# Anti-ligand–induced binding sites (LIBS) single-chain antibody conjugated to microbubbles

Chemical name: | Anti-ligand–induced binding sites (LIBS) single-chain antibody conjugated to microbubbles
Abbreviated name: | LIBS-MBs
Synonym: | LIBS-scFv-MBs
Agent category: | Antibody, single-chain
Target: | Platelet glycoprotein GPIIb/IIIa receptor (CD61/CD41)
Target category: | Receptor
Method of detection: | Ultrasound
Source of signal: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MB)]

Ultrasound is a widely used imaging modality (1), and its role in noninvasive molecular imaging with ligand-carrying microbubbles (MBs) is expanding (2). MBs are spherical cavities encapsulated in a shell and filled with a gas. The shells are made of phospholipids, surfactants, denatured human serum albumin, or synthetic polymers. Ligands and antibodies can be incorporated into the MB shell surface. MBs are usually 2–8 μm in size. MBs of this size provide a strongly reflective interface and resonate to ultrasound waves. They are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (2-4). They also have potential use for drug and gene delivery (5).

Thrombosis plays a major role in many cardiovascular diseases, such as myocardial infarction, pulmonary embolism (PE), deep venous thrombosis (DVT), atherothrombosis, and cerebral venous thrombosis (6, 7). DVT is a significant cause of PE, which is a potentially life-threatening clinical problem. Thrombosis occurs when platelets deposit in regions of low flow in the deep venous system, followed by an activation process of thrombin, which then converts fibrinogen into fibrin. Platelets become activated and bind to fibrinogen, resulting in platelet aggregation via the platelet integrin GPIIb/IIIa (α_IIb_β_3_, CD61/CD41). The thrombus may become organized or detached from the vessel wall. The single-chain antibody (scFv) anti-LIBS was developed to recognize the ligand-induced binding sites (LIBS) epitope of GPIIb/IIIa on the platelets that become exposed only upon activation (8). Anti-LIBS scFv does not bind to circulating platelets. Anti-LIBS scFv was conjugated to microbubbles (MBs) to form LIBS-MBs for ultrasound imaging of platelet-containing thrombi (9).

### Related Resource Links:

- Chapters in MICAD (GPIIb (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=GPIIb+AND+micad%5Bbook%5D), thrombus (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=Thrombus+AND+micad%5Bbook%5D))
- Gene information in NCBI (GPIIIa/CD61 (http://www.ncbi.nlm.nih.gov/gene/3690), GPIIb/CD41 (http://www.ncbi.nlm.nih.gov/gene/3674))
- Articles in Online Mendelian Inheritance in Man (OMIM) (GPIIIa/CD61 (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=173470), GPIIb/CD41 (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=607759))
- Clinical trials (integrin (http://www.clinicaltrials.gov/ct2/results?term=integrin))
- Drug information in FDA (integrin (http://google2.fda.gov/search?q=integrin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=17&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MB+and+synthesis)]

For targeted MBs, Wang et al. (9) prepared biotinylated MBs by sonication of an aqueous dispersion of decafluorobutane gas, distearoylphosphatidylcholine, polyoxyethylene-40-stearate, and distearoylphosphatidylethanolamine-polyethyleneglycol-biotin. MBs were conjugated with scFv-AviTag against LIBS (scFv_anti-LIBS_-AviTag) or nontargeted mut-scFv (scFv_mut_-AviTag) via binding to biotin of the MBs. The addition of scFv-AviTag antibodies to MBs (LIBS-MBs and scFv_mut_-MBs) was verified with flow cytometry, immunofluorescence staining, SDS-PAGE, and Western blot. The diameters of the MBs and the number of scFv antibodies per MBs were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MB+and+in+vitro)]

Flow cytometry analysis showed that scFv_mut_-AviTag had no binding to activated or nonactivated platelets (1.48 AU versus 1.50 AU) (9). On the other hand, scFv_anti-LIBS_-AviTag exhibited a significant increase (P < 0.001) in binding in activated platelets (24.69 AU) compared with nonactivated platelets (2.69 AU). LIBS-MBs, control scFv_mut_-MBs, and non-conjugated MBs perfused through the flow chamber coated with activated platelets at shear rates of 50, 1,000, and 6,000 seconds−^1^, respectively. The numbers of attached LIBS-MBs were 84 ± 10, 81 ± 4, and 74 ± 5, respectively. On the other hand, the numbers of attached control scFv_mut_-MBs were 13 ± 2, 8 ± 1, and 3 ± 1, respectively; the numbers of attached MBs were 15 ± 2, 8 ± 1, and 2 ± 1, respectively. The results showed that LIBS-MBs remained firmly attached to the activated platelets, whereas the majority of scFv_mut_-MBs and MBs were dislodged. Preincubation with excess scFv_anti-LIBS_ led to a significant reduction of attachment of LIBS-MBs to the same background levels as that of the scFv_mut_-MBs and MBs (P < 0.001). Similar flow chamber results were obtained with activated platelets in microthrombi.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MB+and+rodentia)]

Wang et al. (9) performed in vivo ultrasound imaging of thrombosis and thrombolysis in mice (n = 8–10 mice/group) exposed to 6% ferric chloride solution to injure the carotid artery. Videos and images were acquired before and at several time points after intravenous injection of 1.5 × 10^7^ LIBS-MBs, scFv_mut_-MBs, or MBs. The decibel values of the thrombi on the carotid artery were analyzed before and after injection. LIBS-MBs displayed a significant increase in decibels at 20 min compared with scFv_mut_-MBs or MBs (9.6 ± 1.7 versus 1.5 ± 1.3 versus 2.0 ± 1.4 dB, respectively; P < 0.01). Thrombolysis was induced with injection of urokinase plasminogen activator. To monitor thrombolysis, ultrasound imaging sequences were performed every 5 min for 60 min after injection of LIBS-MBs or saline (n = 3/group). The thrombus size, based on ultrasound images with LIBS-MBs, decreased by 40%–60%, whereas no decrease in thrombus size was observed with saline injection (P < 0.05–0.001). Furthermore, grayscale intensity of the thrombi also decreased with LIBS-MBs but not with saline injection (P < 0.05–0.001). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MB+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MB+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=LIBS%20MB+and+human)]

No publication is currently available.

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
5 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
6 Corti R., Fuster V. (2003). New understanding, diagnosis, and prognosis of atherothrombosis and the role of imaging. Am J Cardiol.
7 Taillefer R. (2001). Radiolabeled peptides in the detection of deep venous thrombosis. Semin Nucl Med.
8 Schwarz M., Meade G., Stoll P., Ylanne J., Bassler N., Chen Y.C., Hagemeyer C.E., Ahrens I., Moran N., Kenny D., Fitzgerald D., Bode C., Peter K. (2006). Conformation-specific blockade of the integrin GPIIb/IIIa: a novel antiplatelet strategy that selectively targets activated platelets. Circ Res.
9 Wang X., Hagemeyer C.E., Hohmann J.D., Leitner E., Armstrong P.C., Jia F., Olschewski M., Needles A., Peter K., Ahrens I. (2012). Novel single-chain antibody-targeted microbubbles for molecular ultrasound imaging of thrombosis: validation of a unique noninvasive method for rapid and sensitive detection of thrombi and monitoring of success or failure of thrombolysis in mice. Circulation.